# (+)-2-Hydroxy-3-isobutyl-9-(3-[^18^F]fluoropropoxy)-10-methoxy-1,2,3,4,6,7-hexahydro-11bH-benzo[a]quinolizine

Chemical name: | (+)-2-Hydroxy-3-isobutyl-9-(3-[^18^F]fluoropropoxy)-10-methoxy-1,2,3,4,6,7-hexahydro-11bH-benzo[a]quinolizine
Abbreviated name: | [^18^F]FP-(+)-DTBZ, [^18^F]AV-133
Synonym: | [^18^F]FP-(+)-Dihydrotetrabenazine
Agent category: | Compound
Target: | Type 2 vesicular monoamine transporter (VMAT2)
Target category: | Transporter
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DTBZ%20and%20fluorine%20radioisotopes)]

Vesicular monoamine transporter (VMAT2) is present in brain monoaminergic neurons and is responsible for collecting neurotransmitters (dopamine, norepinephrine, and serotonin) from the cytoplasm and storing them in vesicles for synaptic release (1). VMAT2 is therefore an essential regulator of monoaminergic neuronal function. In the brain, VMAT2 is highly present in the striatum, hypothalamus, substantia nigra, and hippocampus, with low levels in the cerebellum and occipital cortex (2). In the striatum, >95% of VMAT2 is associated with dopaminergic neurons (3). Decreases in the VMAT2 level are implicated in movement disorders such as Parkinson’s disease (PD), Alzheimer’s disease (AD), and Huntington’s disease (HD).

VMAT2 is highly expressed by β cells of the endocrine pancreas and not in exocrine pancreas. VMAT2 is expressed mainly on the β-cells in the islets of Langerhans and composed of 1-2% of the pancreatic mass. β-cell mass (BCM) is a useful indicator of the function of the pancreas. In type I diabetes, β-cells are destroyed leading to a dramatic decrease in BCM. In type II diabetes, there is a slow and insidious decrease in BCM because of peripheral insulin resistance and increase demand for insulin. Decreases in BCM in the human and monkey pancreases correlate to the decreases in insulin level in the blood. VMAT2 is a potential target for non-invasive assessment of BCM and pancreatic function.

VMAT2 has been studied in vivo by positron emission tomography (PET) using [^11^C]dihydrotetrabenazine (2-hydroxy-3-isobutyl-9-[^11^C]methoxy-10-methoxy-1,2,3,4,6,7-hexahydro-11bH-benzo[a]quinolizine, also known as [^11^C]DTBZ) with selective VMAT2 binding activity in neurons. Binding of DTBZ to the vesicular monoamine transporter is stereospecific (4). The (+)-enantiomer showed a high affinity for in vitro binding for to the VMAT2 in rat brain striatum (K_i_ = 0.97 ± 0.48 nM), whereas the (-)-enantiomer was inactive (K_i_ = 2.2 ± 0.3 μM). [^11^C]DTBZ was developed as a PET agent for the non-invasive study of VMAT2 in the human brain and pancreas. To further improve the availability of PET imaging for VMAT2 neurons in the brain and pancreas, ^18^F-labeled analogs of DTBZ have been developed to provide a longer physical half-life of ^18^F (110 min) versus^11^C (20 min) (5).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=VMAT2+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (VMAT2 (http://www.ncbi.nlm.nih.gov/gene/6571))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/193001)
- Clinical trials (VMAT2 (http://www.clinicaltrials.gov/ct2/results?term=VMAT2))
- Drug information in FDA (VMAT2 (http://google2.fda.gov/search?q=VMAT2&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DTBZ%20fluorine%20radioisotopes%20and%20synthesis)]

In the report by Goswami et al. (5), (±)-2-hydroxy-3-isobutyl-9-(3-[^18^F]fluoropropoxy)-10-methoxy-1,2,3,4,6,7-hexahydro-11bH-benzo[a]quinolizine ([^18^F]FP-(±)-DTBZ) was synthesized by a [^18^F]fluoride nucleophilic displacement of the corresponding mesylate precursor in the presence of Kryptofix 2.2.2/K_2_CO_3_. [^18^F]Fluoroethyl-DTBZ ([^18^F]FE-(±)-DTBZ) was similarly prepared. Purification with high-performance liquid chromatography provided good radiochemical yields of 30–40% (decay-corrected), excellent radiochemical purity (>99%), and high specific activity of 74 GBq/μmol (2.0 Ci/μmol) in 50–55 min. Zhu et al. (6) reported synthesis of [^18^F]FP-(+)-DTBZ via an automated module with radiochemical yield of 21-41% (decay-corrected, n = 10) and radiochemical purity of >95% in 40 min. The corresponding tosylate (+)-precursor was employed for the [^18^F]-fluorination.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DTBZ%20fluorine%20radioisotopes%20and%20in%20vitro)]

Henry et al. (2) reported that saturation binding experiments of [^3^H]DTBZ in the synaptic vesicles from murine striata provided an estimated K_d_ value of 2.3 to 2.7 nM, with a B_max_ value of 1.35 pmol/mg protein. In vitro binding studies by Goswami et al. (5) of mouse striatal homogenates provided K_d_ values of 0.52 and 0.48 nM for [^18^F]FE-(±)-DTBZ and [^18^F]FP-(±)-DTBZ, respectively. Goswami et al. (5) also reported that in vitro autoradiography studies of mouse brain slices indicated a selective binding of [^18^F]FP-(±)-DTBZ to the caudate putamen, olfactory tubercle, and nucleus accumbens, which is consistent with VMAT2 distribution. Tetrabenazine (TBZ), a VMAT2 inhibitor, abolished their binding for [^18^F]FP-(±)-DTBZ. Kung et al. reported that K_i_ values were 0.19, 0.10, and >3,000 nM for FP-(±)-DTBZ, FP-(+)-DTBZ (AV-133), and FP-(-)-DTBZ using rat striatal homogenates and [^3^H]TBZ, respectively.

Tsao et al. (7) reported that saturation binding experiments of [^18^F]FP-(+)-DTBZ in the synaptic vesicles from rat β-cells provided two binding sites: site A: K_d_ value of 6.76 ± 1.08 nM with a B_max_ value of 60 ± 10 fmol/mg protein; site B: K_d_ value of 241.5 ± 7.8 nM with a B_max_ value of 1,500 ± 20 fmol/mg protein. A single low affinity binding site (K_d_ value of 208.9 ± 22.5 nM with a B_max_ value of 74.4 ± 1.9 fmol/mg protein) was found using exocrine homogenates. In the rat striatal homogenates, a single high affinity binding site (K_d_ value of 0.19 nM with a B_max_ value of 45 fmol/mg protein) was found.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DTBZ%20fluorine%20radioisotopes%20and%20rodentia)]

Goswami et al. (5) performed ex vivo biodistribution studies in normal mice that demonstrated accumulation of radioactivity in the liver, kidney, spleen, lung, brain, and heart at 2 min after injection of [^18^F]FE-(±)-DTBZ or [^18^F]FP-(±)-DTBZ, with a gradual washout in all organs. Both tracers entered the brain readily with 4.66% and 7.08% injected dose/g (ID/g) for [^18^F]FE-(±)-DTBZ and [^18^F]FP-(±)-DTBZ at 2 min, respectively. [^18^F]FP-(±)-DTBZ exhibited a faster brain washout than [^18^F]FE-(±)-DTBZ (13% versus >50% remaining at 30 min, respectively). [^18^F]FP-(±)-DTBZ exhibited a higher accumulation of radioactivity in the bone than [^18^F]-FE-(±)-DTBZ, which indicates a faster defluorination for [^18^F]FP-(±)-DTBZ. [^18^F]FP-(±)-DTBZ accumulation was higher in the striatum (3.84% ID/g) and hippocampus (2.55% ID/g) and lower in the cortex (1.45% ID/g) and cerebellum (1.30% ID/g) at 30 min after injection, with a striatum/cerebellum ratio of 3.0 at 30 min. On the other hand, [^18^F]FE-(±)-DTBZ exhibited a striatum/cerebellum ratio of 1.7 at 30 min. Coinjection of DTBZ (3 mg/kg) with [^18^F]FP-(±)-DTBZ reduced binding to the striatum, hippocampus, and cortex to the background level of the cerebellum, whereas little inhibition was observed in the other organs studied. On the other hand, coinjection of 1.2 mg/kg raclopride (a dopamine D_2/3_ antagonist) with [^18^F]FP-(±)-DTBZ showed no effect on the striatum/cerebellum ratio. Further biodistribution studies in mice by Kung et al. (8) showed the active enantiomer [^18^F]FP-(+)-DTBZ (AV-133) is a sensitive and selectively tracer for VMAT2 imaging with a higher striatum/cerebellum ratio (4.5) than the racemic tracer (3.0).

Kung et al. (9) performed ex vivo biodistribution studies in normal rats that demonstrated accumulation of radioactivity in the pancreas (5.50 ± 0.97% ID/g), liver (2.82 ± 0.24% ID/g), striatum (2.25 ± 0.48% ID/g), kidney (1.06 ± 0.06% ID/g), spleen (1.03 ± 0.18% ID/g), lung (0.69 ± 0.03% ID/g), and heart (0.41 ± 0.03% ID/g) at 30 min after injection of [^18^F]FP-(+)-DTBZ. A gradual washout was observed in all organs except the pancreas. The radioactivity level in the blood was low (0.23 ± 0.06% ID/g). The accumulation of the inactive enantiomer [^18^F]FP-(-)-DTBZ in the pancreas (1.23% ID/g) and striatum (0.16% ID/g) was low at 30 min after injection. Pretreatment with FP-(+)-DTBZ (3.5 mg/kg, 5 min) reduced the radioactivity by 73% and 85% in the pancreas and striatum at 30 min after injection, respectively. PET imaging in rats showed that the pancreas was clearly visualized as the organ with the highest radioactivity at 30-40 min after injection of [^18^F]FP-(+)-DTBZ.

Singhal et al. (10) evaluated [^18^F]FP-(+)-DTBZ PET imaging in a rodent model of diabetes in rats (treated with streptozotocin (STZ) to induced BCM loss and diabetes). Imaging sessions were performed at 13 – 96 h after STZ treatment. Pancreatic standard uptake value (SUV) was observed to decrease with the progressive loss of pancreatic insulin content (R^2^ = 0.366, p = 0.002) as well as BCM loss (R^2^ = 0.470, p = 0.0002). Displacement studies were performed with ~5,500-fold excess FP-(+)-DTBZ (2.5 mg/kg) in control rats (n = 9) and STZ diabetic rats (n = 6) at 90 min after [^18^F]FP-(+)-DTBZ injection. The SUV values were ~7.3 for the control pancreases and ~5.3 for the STZ pancreases. These SUV values were reduced to 2.7 for the control pancreases and 2.5 for the STZ pancreases after displacement.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DTBZ%20fluorine%20radioisotopes%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DTBZ%20fluorine%20radioisotopes%20and%20%28primate%20not%20human%29)]

Kilbourn et al. (11) performed PET imaging in one rhesus monkey to obtain calculated striatal distribution volume ratios (DVR) relative to cerebellum. The striatal DVR values for [^11^C]-(+)-DTBZ, [^18^F]FP-(±)-DTBZ and [^18^F]FP-(+)-DTBZ were 4.54, 3.32, and 6.20, respectively. Administration of TBZ at 40 min after injection of [^18^F]FP-(+)-DTBZ exhibited a rapid loss of radioactivity in the striatum, thalamus and raphe but no change in the cerebellum and cortex.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DTBZ%20fluorine%20radioisotopes%20and%20human)]

Lin et al. (12) performed radiation dosimetry in nine healthy human subjects after injection of 391 MBq (10.6 mCi) of [^18^F]FP-(+)-DTBZ. The radioactivity uptake in the brain was the highest at 7.5% ± 0.6% injected dose at 10 min after injection. High absorbed doses were found in the pancreas, brain, liver and upper large intestine wall. The organ with the highest radiation dose was the pancreas, which received 153.3 ± 23.8 µGy/MBq. The effective dose equivalent and effective dose for [^18^F]FP-(+)-DTBZ were 36.5 ± 2.8 and 27.8 ± 2.5 µSv/MBq, respectively.

## NIH Support

EB 002171, NS 015655, UL1 RR024139, 01 MH068782, R01 NS049438

## References

1 Schuldiner S. (1994). A molecular glimpse of vesicular monoamine transporters. J Neurochem.
2 Henry J.P., Scherman D. (1989). Radioligands of the vesicular monoamine transporter and their use as markers of monoamine storage vesicles. Biochem Pharmacol.
3 Vander Borght T.M., Sima A.A., Kilbourn M.R., Desmond T.J., Kuhl D.E., Frey K.A. (1995). [3H]methoxytetrabenazine: a high specific activity ligand for estimating monoaminergic neuronal integrity. Neuroscience.
4 Kilbourn M., Lee L., Vander Borght T., Jewett D., Frey K. (1995). Binding of alpha-dihydrotetrabenazine to the vesicular monoamine transporter is stereospecific. Eur J Pharmacol.
5 Goswami R., Ponde D.E., Kung M.P., Hou C., Kilbourn M.R., Kung H.F. (2006). Fluoroalkyl derivatives of dihydrotetrabenazine as positron emission tomography imaging agents targeting vesicular monoamine transporters. Nucl Med Biol.
6 Zhu L., Liu Y., Plossl K., Lieberman B., Liu J., Kung H.F. (2010). An improved radiosynthesis of [18F]AV-133: a PET imaging agent for vesicular monoamine transporter 2. Nucl Med Biol.
7 Tsao H.H., Lin K.J., Juang J.H., Skovronsky D.M., Yen T.C., Wey S.P., Kung M.P. (2010). Binding characteristics of 9-fluoropropyl-(+)-dihydrotetrabenzazine (AV-133) to the vesicular monoamine transporter type 2 in rats. Nucl Med Biol.
8 Kung M.P., Hou C., Goswami R., Ponde D.E., Kilbourn M.R., Kung H.F. (2007). Characterization of optically resolved 9-fluoropropyl-dihydrotetrabenazine as a potential PET imaging agent targeting vesicular monoamine transporters. Nucl Med Biol.
9 Kung M.P., Hou C., Lieberman B.P., Oya S., Ponde D.E., Blankemeyer E., Skovronsky D., Kilbourn M.R., Kung H.F. (2008). In vivo imaging of beta-cell mass in rats using 18F-FP-(+)-DTBZ: a potential PET ligand for studying diabetes mellitus. J Nucl Med.
10 Singhal, T., Y.S. Ding, D. Weinzimmer, M.D. Normandin, D. Labaree, J. Ropchan, N. Nabulsi, S.F. Lin, M.B. Skaddan, W.C. Soeller, Y. Huang, R.E. Carson, J.L. Treadway, and G.W. Cline, Pancreatic Beta Cell Mass PET Imaging and Quantification with [(11)C]DTBZ and [ (18)F]FP-(+)-DTBZ in Rodent Models of Diabetes. Mol Imaging Biol, 2010
11 Kilbourn M.R., Hockley B., Lee L., Hou C., Goswami R., Ponde D.E., Kung M.P., Kung H.F. (2007). Pharmacokinetics of [(18)F]fluoroalkyl derivatives of dihydrotetrabenazine in rat and monkey brain. Nucl Med Biol.
12 Lin K.J., Weng Y.H., Wey S.P., Hsiao I.T., Lu C.S., Skovronsky D., Chang H.P., Kung M.P., Yen T.C. (2010). Whole-body biodistribution and radiation dosimetry of 18F-FP-(+)-DTBZ (18F-AV-133): a novel vesicular monoamine transporter 2 imaging agent. J Nucl Med.